# ^125^I-Labeled monoclonal antibody (mAb) 806 targeting the epidermal growth factor receptor deletion variant de2-7 (EGFRvIII)

Chemical name: | ^125^I-Labeled monoclonal antibody (mAb) 806 targeting the epidermal growth factor receptor deletion variant de2-7 (EGFRvIII)
Abbreviated name: | [^125^I]-mAb806
Synonym:
Agent Category: | Antibody
Target: | Epidermal growth factor receptor deletion variant de2-7 (EGFRvIII)
Target Category: | Receptor
Method of detection: | Single-photon emission tomography (SPECT); gamma planar imaging
Source of signal / contrast: | ^125^I
Activation: | No
Studies: | - In vitro; - Rodents | No structure information available in PubChem (http://pubchem.ncbi.nlm.nih.gov/).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=ch806&cmd=DetailsSearch)]

The biological characteristics, activating ligands, and functioning of the different members of the transmembrane epidermal growth factor receptor (EGFR) family are described elsewhere (1-3). These receptors are known to regulate the growth, survival, differentiation, and migration of cells through the activation of an associated intracellular tyrosine kinase (TK) signaling pathway, and they are overexpressed in many malignant epithelial tumors (1, 2). In addition, overexpression of the EGFR usually indicates a poor clinical prognosis for the patient (4). Overexpression of the EGFR in the tumors has been attributed to gene amplification, and this phenomenon is believed to introduce mutations in the receptor (2, 4). The most common mutation observed in the EGFR receptor is the deletion of a segment of the EGFR extracellular domain, including the ligand-binding region, which results in the generation of an EGFR variant known as the de2-7 EGFR or EGFRvIII (2, 4). The generation, structure, functions, and role of EGFRvIII in tumor malignancy have been reviewed by Gan et al. (5). Although EGFRvIII is nonresponsive to the ligand, it is constitutively active with a constantly operating downstream TK signal transduction pathway that appears to promote the development of a neoplastic phenotype, particularly for glioblastoma and to some extent for other cancers such as those of the prostate and the breast (2, 6).

Because the EGFR promotes and helps maintain the cancerous state of cells, several antibodies that inhibit the receptor activity and small molecules that block the downstream TK signaling pathway have been developed and have been approved by the United States Food and Drug Administration (FDA) for the treatment of certain cancers (2). The antibodies are directed toward the extracellular domain of the receptor, block ligand binding, and inhibit activation of the TK signal transduction pathway, which ultimately results in downregulation of the EGFR on the cell surface. However, because the EGFRvIII lacks the ligand-binding region on the extracellular domain, these antibodies cannot obstruct the constitutive mutant receptor activity (2). As a consequence, the monoclonal antibody (mAb) 806, which specifically targets the EGFRvIII, was generated and characterized in preclinical studies (7, 8). Subsequently, a chimeric form of the mAb (chAb), designated as ch806, was developed and evaluated in a phase I clinical trial with patients having cancerous tumors overexpressing the EGFRvIII (4). Results obtained from this trial indicated that ch806 could be a good biotherapeutic agent for the treatment of cancers expressing the ch806 antigen (4). In addition, several other clinical trials (http://clinicaltrials.gov/ct2/results?term=EGFRvIII+) approved by the FDA are in progress to evaluate the targeting of EGFRvIII as a treatment against various cancers.

The internalization, intracellular trafficking, and biodistribution (in nude mice bearing xenograft human epidermoid carcinoma cell tumors) of mAb806 labeled with ^111^In ([^111^In]-mAb806) and ^125^I ([^125^I]-mAb806) have been investigated by Perera et al. (8). The characterization and biodistribution (in nude mice bearing xenograft human glioblastoma cell tumors) of ch806 labeled with ^125^I and ^111^In, respectively, are described in separate chapters in MICAD (www.micad.nih.gov) (9, 10). Another chapter describes the use of ^124^I-labeled ch806 for the detection of EGFRvIII-expressing xenograft human glioblastoma tumors in nude mice with an immuno–positron emission tomography (PET) technique (11). This chapter describes the studies performed with [^125^I]-mAb806. Studies performed with [^111^In]-mAb806 are described in a separate chapter in MICAD (12).

### Other sources of information

Human EGFR Gene (http://www.ncbi.nlm.nih.gov/gene/1956) (Gene ID: 1956)

Protein and mRNA sequence (http://www.ncbi.nlm.nih.gov/nuccore/NM_005228.3) of human EGFR variant 1

EGFR in OMIM (http://www.ncbi.nlm.nih.gov/omim/131550) (Online Mendelian Inheritance in Man)

EGFR signaling pathways (http://pid.nci.nih.gov/search/pathway_landing.shtml?what=graphic&jpg=on&pathway_id=200131&source=NATURE&output-format=graphic&ppage=1&genes_a=1956) (NCI-Nature Pathways Interaction Database)

Anti-EGFR antibodies (http://www.ncbi.nlm.nih.gov/pubmed?term=anti-EGFR%20antibodies&cmd=DetailsSearch) in PubMed

EGFR tyrosine kinase inhibitors (http://www.ncbi.nlm.nih.gov/pubmed?term=egfr%20tyrosine%20kinase%20inhibitors&cmd=DetailsSearch) in PubMed

Related chapters (http://www.ncbi.nlm.nih.gov/sites/entrez?db=Books&cmd=Search&term=EGFR+AND+micad%5Bbook%5D&doptcmdl=TOCView&log%24=booksrch&bname=micad) in MICAD

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=124I-IMP-R4-ch806%20synthesis&cmd=DetailsSearch)]

The labeling of mAb806 with ^125^I was done using a modified chloramine-T method as described by Perera et al. (8). The radiochemical purity of the ^125^I-labeled mAb was reported to be 99.6% as determined with instant thin-layer chromatography. The yield of the radiolabeling reaction was not reported. The specific activity of [^125^I]-mAb806 was reported to be ~37.0 kBq/6.6 pmol (151.5 Ci/mmol). The final formulation and storage conditions of the labeled mAb were not reported.

For use as a control, another isotype-matched mAb, 100-310 (directed against the human A33 antigen), was labeled with ^125^I in a similar manner (8).

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=124I-IMP-R4-ch806%20in%20vitro&cmd=DetailsSearch)]

The immunoreactivity of [^125^I]-mAb806 was determined using A431 cells (a human epidermoid carcinoma cell line that expresses the EGFRvIII receptor) (8). The number of labeled mAb molecules bound per cell was reported to be 3.14 × 10^5^, which is similar to the number determined for [^111^In]-mAb806 (3.89 × 10^5^/cell) (8). The isotype-matched ^125^I-labeled mAb 100-310 did not bind to the A431 cells under the same study conditions.

In another study, the internalization and trafficking of a fluorescent dye (Cy-3)–tagged mAb806 (mAb806-Cy3) was investigated using A431 cells (8). This study revealed that mAb806-Cy3 was internalized by the cells through a dynamin-dependent, clathrin-mediated, endocytotic process. The mAb was initially localized in the endosomes and later trafficked to and accumulated in the lysosomes (8).

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=124I-IMP-R4-ch806%20rodentia&cmd=DetailsSearch)]

The biodistribution of [^125^I]-mAb806 was studied in BALB/c nude mice bearing xenograft A431 cell tumors (8). The animals were injected with the labeled mAb through the tail vein, and the mice were euthanized at predetermined time points (n = 4 animals/time point) for the collection of all major organs, including the tumors (6). In general, the uptake of label from [^125^I]-mAb806 by the tumors was lower than that from the [^111^In]-mAb806 at all time points (8). With [^125^I]-mAb806, the accumulation of radioactivity in the tumors decreased from 13.7 ± 3.3% injected dose per gram tissue (% ID/g) at 4 h post-injection (p.i.) to 9.9 ± 3.5% ID/g at 48 h and reduced to 2.5 ± 6.3% ID/g by 168 h p.i. During the same time period, radioactivity in the blood from [^125^I]-mAb806 was observed to reduce from 29.8 ± 1.7% ID/g at 4 h p.i. to 12.5 ± 1.7% ID/g at 48 h p.i., and to further reduce to 4.7 ± 1.6 at 168 h p.i. To compare the accumulation of radioactivity from [^125^I]-mAb806 and [^111^In]-mAb806, respectively, in the tumors and blood of the animals, the reader is referred to Table 1 in Perera et al. (8). All major organs were reported to have an accumulation of <10% ID/g radioactivity from [^125^I]-mAb806 at all time points. No blocking studies using unlabeled mAb806 or another suitable anti-EGFR mAb were reported.

On the basis of results obtained from these studies, the investigators concluded that [^111^In]-mAb806 would be a better candidate than [^125^I]-mAb806 for development as a cancer detection or therapeutic agent (8).

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=111In-mAb%20806%20Non-Primate%20Mammals&cmd=DetailsSearch)]

No references are currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=111In-mAb%20806%20Non-Human%20Primates&cmd=DetailsSearch)]

No references are currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=111In-mAb%20806%20Human%20Studies&cmd=DetailsSearch)]

No references are currently available.

## Supplemental Information

[Disclaimers]

No information is currently available.

## References

1 Spector N.L., Blackwell K.L. (2009). Understanding the mechanisms behind trastuzumab therapy for human epidermal growth factor receptor 2-positive breast cancer. J Clin Oncol.
2 Pines G., Kostler W.J., Yarden Y. (2010). Oncogenic mutant forms of EGFR: lessons in signal transduction and targets for cancer therapy. FEBS Lett.
3 Hasselbalch, B., U. Lassen, H.S. Poulsen, and M.T. Stockhausen, Cetuximab Insufficiently Inhibits Glioma Cell Growth Due to Persistent EGFR Downstream Signaling. Cancer Invest. 2010
4 Scott A.M., Lee F.T., Tebbutt N., Herbertson R., Gill S.S., Liu Z., Skrinos E., Murone C., Saunder T.H., Chappell B., Papenfuss A.T., Poon A.M., Hopkins W., Smyth F.E., MacGregor D., Cher L.M., Jungbluth A.A., Ritter G., Brechbiel M.W., Murphy R., Burgess A.W., Hoffman E.W., Johns T.G., Old L.J. (2007). A phase I clinical trial with monoclonal antibody ch806 targeting transitional state and mutant epidermal growth factor receptors. Proc Natl Acad Sci U S A.
5 Gan H.K., Kaye A.H., Luwor R.B. (2009). The EGFRvIII variant in glioblastoma multiforme. J Clin Neurosci.
6 Lee F.T., O'Keefe G.J., Gan H.K., Mountain A.J., Jones G.R., Saunder T.H., Sagona J., Rigopoulos A., Smyth F.E., Johns T.G., Govindan S.V., Goldenberg D.M., Old L.J., Scott A.M. (2010). Immuno-PET quantitation of de2-7 epidermal growth factor receptor expression in glioma using 124I-IMP-R4-labeled antibody ch806. J Nucl Med.
7 Jungbluth A.A., Stockert E., Huang H.J., Collins V.P., Coplan K., Iversen K., Kolb D., Johns T.J., Scott A.M., Gullick W.J., Ritter G., Cohen L., Scanlan M.J., Cavenee W.K., Old L.J. (2003). A monoclonal antibody recognizing human cancers with amplification/overexpression of the human epidermal growth factor receptor. Proc Natl Acad Sci U S A.
8 Perera R.M., Zoncu R., Johns T.G., Pypaert M., Lee F.T., Mellman I., Old L.J., Toomre D.K., Scott A.M. (2007). Internalization, intracellular trafficking, and biodistribution of monoclonal antibody 806: a novel anti-epidermal growth factor receptor antibody. Neoplasia.
9 Chopra, A., [111In]-Labeled CHX-A"-DTPA conjugated chimeric antibody 806 (ch806) targeting the epidermal growth factor receptor deletion variant de2-7 (EGFRvIII). Molecular Imaging and Contrast agent Database (MICAD) [database online]. National Library of Medicine, NCBI, Bethesda, MD, USA. Available from www.micad.nih.gov, 2004 -to current.
10 Chopra, A., [125I]-Labeled chimeric antibody 806 (ch806) targeting the epidermal growth factor receptor deletion variant de2-7 (EGFRvIII). Molecular Imaging and Contrast agent Database (MICAD) [database online]. National Library of Medicine, NCBI, Bethesda, MD, USA. Available from www.micad.nih.gov, 2004 -to current.
11 Chopra, A., [124I]-Labeled residulizing ligand IMP-R4 conjugated chimeric monoclonal antibody ch806 targeting the epidermal growth factor receptor deletion variant de2-7 (EGFRvIII). Molecular Imaging and Contrast agent Database (MICAD) [database online]. National Library of Medicine, NCBI, Bethesda, MD, USA. Available from www.micad.nih.gov, 2004 -to current.
12 Chopra, A., [111In]-Labeled CHX-A"-DTPA conjugated monoclonal antibody 806 (mAb 806) targeting the epidermal growth factor receptor deletion variant de2-7 (EGFRvIII). Molecular Imaging and Contrast agent Database (MICAD) [database online]. National Library of Medicine, NCBI, Bethesda, MD, USA. Available from www.micad.nih.gov, 2004 -to current.